# Stabilized sulfur hexafluoride microbubbles

Chemical name: | Stabilized sulfur hexafluoride microbubbles
Abbreviated name: | SF_6_ microbubbles
Synonym: | SonoVue^®^, BR1
Agent Category: | Lipid microbubbles
Target: | Nontarget
Target Category: | Nontarget filling of blood vessels and heart chambers
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles and sulfur hexafluoride
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SonoVue)]

Stabilized sulfur hexafluoride microbubbles (SF_6_ microbubbles), a preparation of stabilized microbubbles containing sulfur hexafluoride gas were developed as an ultrasound (US) contrast agent to enhance US images (1, 2). The SF_6_ microbubbles preparation is used clinically in Europe to enhance US image contrast in echocardiography, Doppler macrovasculature, and Doppler microvasculature (3).

US contrast agents, or echopharmaceuticals, are designed to change the attenuation (absorption, reflection, and refraction) or impedance (resistance to sound propagation) of sound to enhance the differentiation of the signal (echo) of a target organ from that of the surrounding tissue (4-7). Gas-liquid emulsions (microbubbles or gaseous particles) are highly echogenic invivo because of the nonlinear rarefaction and compression effects that lead to volume pulsations of microbubbles (5, 8, 9). Human serum albumin, synthetic polymers and phospholipids have been used to construct the membranes of these bubbles. Microbubble preparations of various formulations have been developed, and their clinical usefulness depends greatly on the size and stability of these bubbles in vivo. The potential applications of US agents include US contrast enhancement in heart, liver, kidney, breast, blood vessel, pancreas, spleen and gastrointestinal diseases (10-18). The current clinical application of these agents in the United States is primarily in myocardial contrast echocardiography .

Perfluorocarbons (PFCs) are inert, volatile chemicals and can be encapsulated within microbubbles to provide a stabilizing effect. The extremely low water solubility of PFCs sets up an in vivo equilibrium in the water-soluble gases that diffuse in and out of the microbubble, but the PFC vapor counterbalances the surface tension and blood pressure forces that push the gases inside the bubble toward dissolution. As a result, the combined properties of the microbubble shell and the PFC gas inside determine the stability and output signal of each microbubble in vivo. PFC emulsions were initially studied as oxygen carriers (blood substitutes) (19, 20). Perfluorooctyl bromide (C_8_BrF_17_) was first discovered to possess sufficient lipophilicity to be formulated into stable emulsions, but it was developed as an oral agent for negative magnetic resonance imaging of the gastrointestinal tract (5). Schneider (21) described the development of microbubbles stabilized by phospholipids and a perfluorochemical SF_6_ gas. This SF_6_ microbubbles agent is commercially available in Europe, and it consists of a lyophilized phospholipids/poly(ethylene glycol)/palmitic acid powder stored under SF_6_ gas. Upon addition of a saline solution, a suspension of microbubbles (2.5 μm mean diameter in the range from 0.7 to 10 μm; 2 ×10^8^ microbubbles/ml) stabilized by a lipidic monolayer is produced (5, 21). Microbubbles <2 μm in diameter do not contribute appreciably to the echogenicity at medical US frequencies, but microbubbles that are >6.2 μm in diameter tend to be trapped in the pulmonary circulation (22).

Serious cardiopulmonary reactions following the administration of ultrasound microbubble contrast agents have been reported (23). In 2007, the US FDA (http://www.fda.gov/cder/drug/InfoSheets/HCP/microbubbleHCP.htm) requested that warnings emphasizing the risk for serious cardiopulmonary reactions be added to the labeling of these agents. The uses of these agents are contraindicated in patients with unstable cardiopulmonary status.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Sonovue%20AND%20synthesis)]

PFCs are inert organic materials initially developed for handling the extremely corrosive uranium fluorides (19, 20, 24). Some PFCs are derived directly from the manufacturing line that led to Teflon and other diverse industrial surfactants. Two major strategies are commonly used in producing PFCs. One strategy is substituting fluorine atoms for hydrogen atoms in the parent hydrocarbon analog by electrochemical fluorination, fluorination by high-valence metal fluorides, or direct fluorination. Another strategy is combining smaller, reactive fluorinated building blocks by telomerization. SF_6_ is a gas at standard conditions and is colorless, odorless, non-toxic, and non-flammable. SF_6_ comprises 6 fluorine atoms attached to a central sulfur atom with an octahedral geometry. SF_6_ can be prepared from the elements by the combustion of sulfur in fluorine (25),

The European commercial preparation of SF_6_ microbubbles is 25 mg of dry, lyophilized powder in an atmosphere of SF_6_ contained in a glass vial with elastomeric closure (1, 3). The lyophilysate is composed of a combination of pharmaceutical grade polyethylene glycol 4000 and phospholipids (distearoylphosphatidylcholine and dipalmitoylphosphatidylglycerol). The agent is prepared immediately before use by injecting 5 ml of normal saline through the septum to the content of the vial. The vial is then shaken vigorously for 20 s after which the desired volume of the dispersion can be drawn. One milliliter of the resulting dispersion contains 8 μl SF_6_ in the microbubbles, equivalent to 45 μg. The bubble concentration of the suspension is between 100 and 500 million microbubbles/ml. The total volume of SF_6_ gas in the bubbles is approximately 5 μl/ml of the reconstituted suspension. The suspension has an osmolarity of 294 mOsm/kg, a pH that is between 4.5 and 7.5, and the viscosity is below 2 mPas.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SonoVue%20AND%20in%20vitro)]

Schneider (21) described the in vitro properties of SF_6_ microbubbles after reconstitution with normal saline. When the suspension was left standing for >15−30 min, the bubbles rose to the surface. The suspension could be easily rehomogenized by gently agitating the vial top to bottom. SF_6_ microbubbles showed a peak in backscatter coefficient (BSC) at about 3 MHz. When the agent was insonating with a 2.25 MHz transducer, the scattering power increased linearly with the mechanical index (i.e., 10 dB/decade). In second harmonics, the scattering power increased with the square of the mechanical index (i.e., 20 dB/decade). Schneider et al. (1) found no changes in the bubble characteristics or in their echogenicity for at least 8 h after reconstitution. SF_6_ microbubbles showed constant echogenic properties over the entire 1−10 MHz frequency range. The BSC was proportional to the bubble concentration over the range 2 × 10^4^ to 3 × 10^5^ bubbles/ml. The critical pressure (Pc; pressure at which absorbance decreased by 50%) was 127 mm Hg. Microbubble preparations with Pc values<60 mm Hg were not useful to opacify the left ventricle.

Using in vitro test phantoms and rabbit liver, Arditi et al. (26) demonstrated that SF_6_ microbubbles had promising contrast-enhancing properties when used in differential contrast echography. In an in vitro study using a tissue-mimicking phantom, Broillet et al. (27) showed that SF_6_ microbubbles were detected in the phantom at 500−700 Hz pulse repetition frequencies (PRFs) when they were circulated at different velocities (1.5−10 cm/s). SF_6_ microbubbles showed stronger contrast effects at higher velocities. Moran et al. (28) studied the in vitro acoustic characteristics of SF_6_ microbubbles at 30 MHz. At concentrations of 0.01−5 million microbubbles/ml, the agent exhibited a linear relationship between log(concentration) and mean backscatter power. At concentrations <0.01 million microbubbles/ml, the mean backscatter levels appeared to reach a plateau.

Rahim et al. (29) used Chinese hamster ovary (CHO) cells to study various factors that affected US/microbubble-mediated gene delivery. β-galactosidase gene delivery was achieved with an efficiency of ~4% to adherent cells at 0.25 MPa acoustic pressure amplitude, 1 kHz PRF and 10 s duration of exposure.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SonoVue%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SonoVue%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Schneider et al. (1) administered SF_6_ microbubbles by i.v.injection in the auricular vein of minipigs to opacify the right and left heart chambers. At doses <0.03 ml/kg, there was a dose-dependent increase of opacification in the left ventricle. No additional increase was found with 0.05−0.2 ml/kg. Extensive acoustic attenuation was observed with doses >0.1 ml/kg. Broillet et al. (27) evaluated SF_6_ microbubbles in minipigs by intermittent harmonic-power Doppler imaging and PRFs. At a dose of 0.01 ml/kg, SF_6_ microbubbles produced a strong and homogeneous myocardial opacification. Higher doses prolonged the duration of the contrast effect. Varying the PRF appeared to allow the detection of perfusion differences within the myocardium during reversible left anterior descending coronary artery occlusion.

The influence of Doppler system settings on the clearance kinetics of SF_6_ microbubbles was reported by Seidel et al. (30). Six dogs were investigated with a transcranial Doppler system. Each dog received 0.03 ml/kg SF_6_ microbubbles by i.v. injection at a rate of 1 ml/s. The Doppler time intensity curve showed a two-phase decrease with a very short distribution phase α and an elimination phase β. Altering the system settings appeared to have a significant effect on the mean peak Doppler intensity.

Kaps et al. (31) studied the pharmacokinetics of SF_6_ microbubbles in dogs. Five dogs received two i.v. infusion rates (35 or 70 ml/h for 7 min) of SF_6_ microbubbles and were imaged by transcranial Doppler. The study demonstrated a dose-dependent level of increased Doppler mean intensity within the brain circulation. The results showed that only the 70-ml/h infusion rate produced a stable level of increased Doppler mean intensity and reached 24 to 26 dB over baseline values. The 35-ml/h infusion rate did not produce a stable level of increased Doppler mean intensity. After infusion termination, time-intensity curves revealed a linear decrease (±0.066 dB/s for 70 ml/h infusion rate) that was not related to the infusion rate.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SonoVue%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SonoVue%20AND%20huma)]

Schneider (21) studied the fate of SF_6_ in human volunteers after a single i.v. administration of 0.3 ml/kg. The blood distribution t_½_ was about 1 min, and the elimination t_½_ was approximately 6 min. More than 80% of SF_6_ gas was excreted through exhalation after 11 min. Morel et al. (32) evaluated the blood kinetics and pulmonary elimination of SF_6_ microbubbles in 12 healthy subjects. Each subject received two i.v. bolus doses of 0.03 and 0.3 ml/kg with 3−14 days between doses. For both doses, the maximum blood concentration was reached within 1−2 min and then rapidly declined. For the lower dose, it was not possible to define the distribution and elimination phases. For the higher dose, the mean distribution t_½_ times were 0.97 min (men) and 1.23 min (women), and the median elimination t_½_ times were 8.25 min (men) and 6.93 min (women). The route of SF_6_ elimination was via the lungs in the exhaled air with approximately 40−50% of the dose being eliminated within the first minute and with >75% of the dose eliminated by 11 min (33). In a study of 12 healthy volunteers, Kaps et al. (34) found that SF_6_ microbubbles were safe, well tolerable, and provided a long-lasting US contrast enhancement in transcranial Doppler sonography.

The safety and tolerability of SF_6_ microbubbles were evaluated in 66 healthy volunteers (doses of 0.003−0.12 ml/kg) during two placebo-controlled phase I studies and 12 patients with chronic obstructive pulmonary disease (COPD; dose of 0.057 ml/kg) during a phase II placebo-controlled study (35). For both phase I and phase II studies, no serious adverse events (AEs) occurred. There were seven nonserious AEs judged as possibly or definitely related to SF_6_ microbubbles in the healthy volunteers, and there were two nonserious AEs reported in the COPD patients. There was one report of local heat at the injection from the healthy volunteers. Torzilli (36) reviewed the adverse effects of SF_6_ microbubbles in 3,212 subjects and reported that the overall incidence of AEs was 7.7% (possible, probably, or unknown relationship to the use of SF_6_ microbubbles), and the incidence of serious AEs was <0.0002%. Rare serious AEs were predominantly hypersensitivity reactions. In 2004, a precautionary and temporary suspension of SF_6_ microbubble use in cardiac studies was issued in Europe because of three case reports of fatal outcomes in patients with a high underlying risk for major cardiac complications. Piscaglia and Bolondi (37) performed a retrospective analysis of 23,188 studies in abdominal examination from 28 Italian centers. No fatal event was reported. The overall rate of all AEs was 0.125%, and the rate of serious AEs was 0.0086%.

In a multicenter evaluation of SF_6_ microbubbles for improved endocardial border delineation, Nanda et al. (12) studied 138 patients with highly suspected cardiac disease. Patients received four bolus injections of 0.5, 1, 2, and 4 ml of SF_6_ microbubbles. Scores of left ventricle opacification (LVO) were significantly higher than the control group with saline injection. Across all doses, 73-93% of patients had moderate to complete LVO. The mean duration of useful contrast effect ranged from 0.8−4.1 min. Opacification was negligible in all patients who received saline injection. Although SF_6_ microbubbles have not been approved by the United States Food and Drug Administration, the safety and efficacy of SF_6_ microbubbles for US contrast enhancement have been studied for the diseases of the heart (176 patients) (12, 33, 38), vascular structures (566 patients) (10, 13, 34), liver (478 patients) (11, 39-43), breast (196 patients) (14), spleen (46 patients), pancreas (cystic pancreatic masses with a different vascularization pattern) (31 patients) (44), and gastrointestinal tract (Crohn’s disease with a thickened bowel wall) (15 patients) (18).

## Supplemental Information

[Disclaimers]

The European Agency for the Evaluation of Medicinal Products May 2004

## References

1 Schneider M., Arditi M., Barrau M.B., Brochot J., Broillet A., Ventrone R., Yan F. (1995). BR1: a new ultrasonographic contrast agent based on sulfur hexafluoride-filled microbubbles. Invest Radiol.
2 Schneider M. (1999). SonoVue, a new ultrasound contrast agent. Eur Radiol.
3 Bracco SONOVUE. (2004). (sulphur hexafluoride) Package Insert. p. 1-9.
4 Morawski A.M., Lanza G.A., Wickline S.A. (2005). Targeted contrast agents for magnetic resonance imaging and ultrasound. Curr Opin Biotechnol.
5 Schutt E.G., Klein D.H., Mattrey R.M., Riess J.G. (2003). Injectable microbubbles as contrast agents for diagnostic ultrasound imaging: the key role of perfluorochemicals. Angew Chem Int Ed Engl.
6. Swanson, D.P., Enhancement agents for ultrasound: Fundamentals, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 682-687.
7. Gobuty, A.H., Perspectives in ultrasound contrast agents, in Contrast media: Biologic effects and clinical application, Z. Parvez, R. Moncada and M. Sovak, Editor. 1987, CRC: Boca Raton, Florida. p. 145-155.
8 Averkiou M., Powers J., Skyba D., Bruce M., Jensen S. (2003). Ultrasound contrast imaging research. Ultrasound Q.
9 Miller A.P., Nanda N.C. (2004). Contrast echocardiography: new agents. Ultrasound Med Biol.
10 Sidhu P.S., Allan P.L., Cattin F., Cosgrove D.O., Davies A.H., Do D.D., Karakagil S., Langholz J., Legemate D.A., Martegani A., Llull J.B., Pezzoli C., Spinazzi A. (2006). Diagnostic efficacy of SonoVue, a second generation contrast agent, in the assessment of extracranial carotid or peripheral arteries using colour and spectral Doppler ultrasound: a multicentre study. Br J Radiol.
11 Nicolau C., Catala V., Vilana R., Gilabert R., Bianchi L., Sole M., Pages M., Bru C. (2004). Evaluation of hepatocellular carcinoma using SonoVue, a second generation ultrasound contrast agent: correlation with cellular differentiation. Eur Radiol.
12 Nanda N.C., Wistran D.C., Karlsberg R.P., Hack T.C., Smith W.B., Foley D.A., Picard M.H., Cotter B. (2002). Multicenter evaluation of SonoVue for improved endocardial border delineation. Echocardiography.
13 Spinazzi A., Llull J.B. (2002). Diagnostic performance of SonoVue-enhanced color duplex sonography of vascular structures. Acad Radiol.
14 Cosgrove D.O., Kedar R.P., Bamber J.C., al-Murrani B., Davey J.B., Fisher C., McKinna J.A., Svensson W.E., Tohno E., Vagios E., Alsanjari N.A. (1993). Breast diseases: color Doppler US in differential diagnosis. Radiology.
15 Rickes S., Uhle C., Kahl S., Kolfenbach S., Monkemuller K., Effenberger O., Malfertheiner P. (2006). Echo enhanced ultrasound: a new valid initial imaging approach for severe acute pancreatitis. Gut.
16 Gorg C., Bert T. (2005). Contrast enhanced sonography of focal splenic lesions with a second-generation contrast agent. Ultraschall Med.
17 Barr R. (2002). Seeking consensus: contrast ultrasound in radiology. Eur J Radiol.
18 De Pascale A., Garofalo G., Perna M., Priola S., Fava C. (2006). Contrast-enhanced ultrasonography in Crohn's disease. Radiol Med (Torino).
19 Riess J.G. (2001). Oxygen carriers ("blood substitutes")--raison d'etre, chemistry, and some physiology. Chem Rev.
20 Riess J.G. (2002). Blood substitutes and other potential biomedical applications of fluorinated colloids. Journal of Fluorine Chemistry.
21 Schneider M. (1999). Characteristics of SonoVuetrade mark. Echocardiography.
22 Gorce J.M., Arditi M., Schneider M. (2000). Influence of bubble size distribution on the echogenicity of ultrasound contrast agents: a study of SonoVue. Invest Radiol.
23 Blomley M., Claudon M., Cosgrove D. (2007). WFUMB Safety Symposium on Ultrasound Contrast Agents: clinical applications and safety concerns. Ultrasound Med Biol.
24 Riess J.G. (2002). Fluorous micro- and nanophases with a biochemical perspective. Tetrahedron.
25 Schumb W.C., Gamble E.L. (1930). The preparation of sulfur hexafluoride and some of its physical properties. Journal of the American Chemical Society.
26 Arditi M., Brenier T., Schneider M. (1997). Preliminary study in differential contrast echography. Ultrasound Med Biol.
27 Broillet A., Puginier J., Ventrone R., Schneider M. (1998). Assessment of myocardial perfusion by intermittent harmonic power Doppler using SonoVue, a new ultrasound contrast agent. Invest Radiol.
28 Moran C.M., Watson R.J., Fox K.A., McDicken W.N. (2002). In vitro acoustic characterisation of four intravenous ultrasonic contrast agents at 30 MHz. Ultrasound Med Biol.
29 Rahim A., Taylor S.L., Bush N.L., ter Haar G.R., Bamber J.C., Porter C.D. (2006). Physical parameters affecting ultrasound/microbubble-mediated gene delivery efficiency in vitro. Ultrasound Med Biol.
30 Seidel G., Vidal-Langwasser M., Algermissen C., Gerriets T., Kaps M. (1999). The influence of Doppler system settings on the clearance kinetics of different ultrasound contrast agents. Eur J Ultrasound.
31 Kaps M., Seidel G., Algermissen C., Gerriets T., Broillet A. (2001). Pharmacokinetics of echocontrast agent infusion in a dog model. J Neuroimaging.
32 Morel D.R., Schwieger I., Hohn L., Terrettaz J., Llull J.B., Cornioley Y.A., Schneider M. (2000). Human pharmacokinetics and safety evaluation of SonoVue, a new contrast agent for ultrasound imaging. Invest Radiol.
33 Bokor D. (2000). Diagnostic efficacy of SonoVue. Am J Cardiol.
34 Kaps M., Seidel G., Bokor D., Modrau B., Algermissen C. (1999). Safety and ultrasound-enhancing potentials of a new sulfur hexafluoride-containing agent in the cerebral circulation. J Neuroimaging.
35 Bokor D., Chambers J.B., Rees P.J., Mant T.G., Luzzani F., Spinazzi A. (2001). Clinical safety of SonoVue, a new contrast agent for ultrasound imaging, in healthy volunteers and in patients with chronic obstructive pulmonary disease. Invest Radiol.
36 Torzilli G. (2005). Adverse effects associated with SonoVue use. Expert Opin Drug Saf.
37 Piscaglia F., Bolondi L. (2006). The safety of Sonovue(R) in abdominal applications: Retrospective analysis of 23188 investigations. Ultrasound Med Biol.
38 Brown A.S., Calachanis M., Evdoridis C., Hancock J., Wild S., Prasan A., Nihoyannopoulos P., Monaghan M.J. (2004). Sonovue improves endocardial border detection and variability in assessing wall motion score and ejection fraction during stress echocardiography. Ir J Med Sci.
39 Lim A.K., Patel N., Eckersley R.J., Goldin R.D., Thomas H.C., Cosgrove D.O., Taylor-Robinson S.D., Blomley M.J. (2006). Hepatic vein transit time of SonoVue: a comparative study with Levovist. Radiology.
40 Leen E., Angerson W.J., Yarmenitis S., Bongartz G., Blomley M., Del Maschio A., Summaria V., Maresca G., Pezzoli C., Llull J.B. (2002). Multi-centre clinical study evaluating the efficacy of SonoVue (BR1), a new ultrasound contrast agent in Doppler investigation of focal hepatic lesions. Eur J Radiol.
41 Leen E., Ceccotti P., Kalogeropoulou C., Angerson W.J., Moug S.J., Horgan P.G. (2006). Prospective multicenter trial evaluating a novel method of characterizing focal liver lesions using contrast-enhanced sonography. AJR Am J Roentgenol.
42 Ricci P., Laghi A., Cantisani V., Paolantonio P., Pacella S., Pagliara E., Arduini F., Pasqualini V., Trippa F., Filpo M., Passariello R. (2005). Contrast-enhanced sonography with SonoVue: enhancement patterns of benign focal liver lesions and correlation with dynamic gadobenate dimeglumine-enhanced MRI. AJR Am J Roentgenol.
43 von Herbay A., Vogt C., Willers R., Haussinger D. (2004). Real-time imaging with the sonographic contrast agent SonoVue: differentiation between benign and malignant hepatic lesions. J Ultrasound Med.
44 Rickes S., Randhan W., Malfertheiner P. (2004). Differentiation of cystic pancreatic lesions by echo-enhanced sonography with pulse inversion imaging - presentation of case reports. Z Gastroenterol.